# TAMRA-IL-13-Conjugated functionalized gadolinium metallofullerene (Gd_3_N@C_80_(OH)_-26_(CH_2_CH_2_COOH)_-16_)

Chemical name: | TAMRA-IL-13-Conjugated functionalized gadolinium metallofullerene (Gd_3_N@C_80_(OH)_-26_(CH_2_CH_2_COOH)_-16_)
Abbreviated name: | TAMRA-IL-13-f-Gd_3_N@C_80_
Synonym:
Agent category: | Nanoparticle
Target: | IL-13 receptor (IL-13Rα2)
Target category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Gadolinium, Gd^3+^
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd%20metallofullerene)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally (1). Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the nuclear density (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field. Cross-linked iron oxide nanoparticles and other iron oxide formulations affect T2 primarily and lead to a decreased signal (2). On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

Glioblastoma multiforme (GBM) is the most common primary malignant brain tumor, with a median survival of ~1 year for GBM patients (3). The GBM tumor is highly invasive and resistant to treatment with radiation and chemotherapy. GBM tissues (~50%) have been reported to overexpress the interleukin-13 receptor α2 subunit (IL-13Rα2) relative to normal brain tissues (4). Debinski et al. (5) identified residues of IL-13 that bind specifically to IL-13Rα2. Fillmore et al. (6) designed a peptide (VDKLLLHLKKLFREGQFNRNFESIIICRDRT-OH, denoted as the IL-13 peptide) based on these residues, then attached a TAMRA fluorescent label and conjugated the IL-13 peptide to a functionalized (carboxylated/hydroxylated) Gd-metallofullerene carbon cage (TAMRA-IL-13-f-Gd_3_N@C_80_). TAMRA-IL-13-f-Gd_3_N@C_80_ has been studied for MRI of IL-13Rα2 expression on glioma tumors in mice.

### Related Resource Links:

- Chapters in MICAD (IL-13 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=IL-13+AND+micad%5Bbook%5D))
- Gene information in NCBI (IL-13 (http://www.ncbi.nlm.nih.gov/gene/3596), IL-13Rα2 (http://www.ncbi.nlm.nih.gov/gene?term=3598))
- Articles in Online Mendelian Inheritance in Man (OMIM) (IL-13 (http://www.ncbi.nlm.nih.gov/omim/147683), IL-13Rα2 (http://www.ncbi.nlm.nih.gov/omim/300130))
- Clinical trials (IL-13 (http://www.clinicaltrials.gov/ct2/results?term=IL13))
- Drug information in FDA (IL-13 (http://google2.fda.gov/search?q=IL-13&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IL-13%20gd%20metallofullerene+synthesis)]

Synthesis of Gd_3_N@C_80_(OH)_-26_(CH_2_CH_2_COOH)_-16_ (f-Gd_3_N@C_80_) was reported by Shu et al. (7). There were 3 Gd^3+^, 26 hydroxyl, and 16 carboxyl moieties per metallofullerene. f-Gd_3_N@C_80_ exhibited a hydrodynamic diameter of ~78 nm. The r1 and r2 relaxivity values (2.4 T) of f-Gd_3_N@C_80_ in phosphate-buffered saline (PBS, pH 7.4) at room temperature were 35 mM−^1^s−^1^ and 62 mM−^1^s−^1^, respectively. Fillmore et al. (6) prepared TAMRA-IL-13-f-Gd_3_N@C_80_ by conjugation of 7.5 nmol TAMRA-IL-13 peptide (4 kDa, obtained from New England Peptide, MA) to f-Gd_3_N@C_80_ (6.5 nmol) in the presence of N-(3-dimethylaminopropyl)-N’-ethylcarbodiimide and N-hydroxysuccinimide in PBS for 18 h at room temperature. Polyacrylamide electrophoresis of TAMRA-IL-13-f-Gd_3_N@C_80_ showed the UV (550 nm excitation) visualization of TAMRA-IL-13 peptide attachment to f-Gd_3_N@C_80_. There were three to four TAMRA-IL-13 peptides per metallofullerene. The hydrodynamic diameter, zeta potential, and in vitro MRI characterization of TAMRA-IL-13-f-Gd_3_N@C_80_ were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IL-13%20gd%20metallofullerene+in%20vitro)]

Fillmore et al. (6) performed cellular uptake studies of TAMRA-IL-13-f-Gd_3_N@C_80_ (1.2 µM) and f-Gd_3_N@C_80_ (1.2 µM) in human glioma U87MG cells. U87MG cells treated with TAMRA-IL-13-f-Gd_3_N@C_80_ accumulated more Gd (882.3 pmol of Gd/10^5^ cells) at 3 h after incubation than did U87MG cells treated with f-Gd_3_N@C_80_ (13.6 pmol of GD/10^5^ cells) at the same time point. The cell viability was not affected by either agent at 3 h and 6 h after incubation. No blocking or in vitro MRI experiments were performed.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IL-13%20gd%20metallofullerene+rodentia)]

Fillmore et al. (6) performed MRI (2.4 T) in nude mice (number of mice not reported) bearing an orthotopic U87MG xenograft. TAMRA-IL-13-f-Gd_3_N@C_80_ (amount administered not reported) was infused intratumorally by convection-enhanced delivery (CED) at 10 d after injection of tumor cells into the brain. There was a bright contrast at the infusion site immediately with T1-weighted MRI, compared to that at 12 h prior to CED infusion. At 24 h after infusion, MRI showed a visible contrast area (2.5 mm in diameter) at the tumor infusion site. Confocal microscopy images of the TAMRA fluorescent signal were co-localized with the tumor lesions. The investigators concluded that further studies are needed to assess the specificity of TAMRA-IL-13-f-Gd_3_N@C_80_ binding to IL-13Rα2.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IL-13%20gd%20metallofullerene+and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IL-13%20gd%20metallofullerene+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IL-13%20gd%20metallofullerene+human)]

No publication is currently available.

## NIH Support

1R01-CA119371 R01 CA119371, 5P30 NS047463

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Pan D., Carauthers S.D., Chen J., Winter P.M., SenPan A., Schmieder A.H., Wickline S.A., Lanza G.M. (2010). Nanomedicine strategies for molecular targets with MRI and optical imaging. Future Med Chem.
3 Kumar H.R., Zhong X., Sandoval J.A., Hickey R.J., Malkas L.H. (2008). Applications of emerging molecular technologies in glioblastoma multiforme. Expert Rev Neurother.
4 Jarboe J.S., Johnson K.R., Choi Y., Lonser R.R., Park J.K. (2007). Expression of interleukin-13 receptor alpha2 in glioblastoma multiforme: implications for targeted therapies. Cancer Res.
5 Debinski W., Obiri N.I., Powers S.K., Pastan I., Puri R.K. (1995). Human glioma cells overexpress receptors for interleukin 13 and are extremely sensitive to a novel chimeric protein composed of interleukin 13 and pseudomonas exotoxin. Clin Cancer Res.
6 Fillmore H.L., Shultz M.D., Henderson S.C., Cooper P., Broaddus W.C., Chen Z.J., Shu C.Y., Zhang J., Ge J., Dorn H.C., Corwin F., Hirsch J.I., Wilson J., Fatouros P.P. (2011). Conjugation of functionalized gadolinium metallofullerenes with IL-13 peptides for targeting and imaging glial tumors. Nanomedicine (Lond).
7 Shu C., Corwin F.D., Zhang J., Chen Z., Reid J.E., Sun M., Xu W., Sim J.H., Wang C., Fatouros P.P., Esker A.R., Gibson H.W., Dorn H.C. (2009). Facile preparation of a new gadofullerene-based magnetic resonance imaging contrast agent with high 1H relaxivity. Bioconjug Chem.